# 4-[^18^F]Fluorobenzoyl-endothelin-1

Chemical name: | 4-[^18^F]Fluorobenzoyl-endothelin-1
Abbreviated name: | [^18^F]ET-1
Synonym: | [^18^F]Endothelin-1
Agent Category: | Polypeptide
Target: | ET receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Endothelin%20-%20I%20human%20studies)]

Endothelin-1 (ET-1) is a 21 amino acid polypeptide that contains two disulfide bonds located closer to the N-terminus. It is believed to have an important role in a variety of physiological processes and contributes to the development of diseases such as atherosclerosis, hypertension, chronic heart failure, pulmonary hypertension, acute and chronic renal failure, etc (1-3). All these effects are mediated through a receptor-ligand mechanism. Two endothelin receptors, ET_A_ and ET_B_, have been identified in mammals (4, 5). Each receptor type is expressed in a variety of tissues, with some tissues expressing both types (6). Various cytokines are known to regulate ET-I expression under physiological conditions (1).

In humans, stimulation of the ET_A_ receptors by ET-1 on underlying smooth muscles of the endothelium causes vasoconstriction that leads to an elevation of blood pressure and the development of hypertension (7, 8). Stimulation of the ET_B_ receptors on the endothelium results in the release of nitric oxide and prostacyclins, which culminates in vasodilation (9). As a result of the involvement of ET-1 in a variety of physiological processes in both normal and diseased states, it is necessary to elucidate the exact role of the ET receptor system in vivo.

Positron emission tomography (PET) is a very sensitive imaging technique, and recent improvements in equipment design have enabled researchers to use it for investigation of the ET receptor system in a small animal model (9-12). ^18^F-Labeled ET-1 ([^18^F]ET-1) was among the first ligands developed for PET study of these receptors in vivo (10, 13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20synthesis)]

Labeling of ET-1 with ^18^F was performed using N-succinimidyl[4-^18^F]fluorobenzoate ([^18^F]SFB) as described by Johnstrom et al. (11). The synthesis of [^18^F]SFB was performed as before (13-15), purified by reverse-phase high-performance liquid chromatography (HPLC) and concentrated in diethyl ether. The ether solution was dehydrated over a bed of magnesium sulfate and evaporated to dryness, and the [^18^F]SFB was dissolved in acetonitrile. ET-1 dissolved in sodium bicarbonate was added to the solution, and the mixture was left at room temperature for 30 min. Radioactive ET was isolated by reverse-phase HPLC and reformulated by the addition of phosphate buffer. The resulting solution was loaded on a C18 SepPak Plus cartridge and the retained labeled ET-1 was eluted in ethanol. The ethanol was evaporated, and [^18^F]ET-1 was dissolved in saline for use in the various studies.

The entire procedure was performed in 207 ± 3 min (n = 20) with a yield of 5.9 ± 0.7%. The final product had a specific activity of 220–370 GBq/µmol (5.94–10 Ci/ µmol) at the end of synthesis and was >95% pure. [^18^F]SFB was shown to label peptides, proteins, and antibodies with ^18^F in the N-terminus or the Ɛ-amino group of the lysine residue (11). Depending on the pH, a mixture of two radiolabeled products may be obtained, with the label either on the N-terminus or the lysine residue at position nine from the N-terminus. With ET-I, performing the reaction under basic conditions (pH 8.6) yielded a single product labeled only at the lysine residue (11).

Confirmation of the purified [^18^F]ET-1 product was performed using mass spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20in%20vitro)]

In vitro binding studies were performed by Johnstrom et al. in human heart and kidney tissues (10) as described by Davenport and Kuc (16). The left ventricle tissue was incubated with 1 nM-labeled ET-1 for an increasing time, 0–120 min, to determine the association rate constant (K_obs_). In the saturation study, the tissue was incubated with increasing concentrations of [^18^F]ET-1 (5 pM–2.5 nM) for 90 min. From these studies it was determined that [^18^F]ET-1 had K_obs_ of 0.045 ± 0.004/min and a half time for association of 17 min. The dissociation constant (K_D_), maximum density of receptors (B_max_), and the Hills coefficient (n_H_) for [^18^F]ET-1 were determined to be 0.43 ± 0.05 nM, 27.8 ± 2.1 fmol/g protein, and 0.95 ± 0.04, respectively.

Kidney sections were used for the competition study (10). The sections were exposed to a fixed concentration of [^18^F]ET-1 in the presence of either FR139317, a selective ET_A_ antagonist, or BQ3020, a selective ET_B_ antagonist. The two antagonists reduced [^18^F]ET-1 binding to the kidney by 33.7 ± 13.3% and 73.3 ± 2.5%, respectively (P<0.05). This indicated that the ET_B_ receptor was the predominant receptor type in the kidney.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20rodentia)]

Johnstrom et al. (11) used microPET to study the in vivo distribution of [^18^F]ET-1 in the rat. For a typical imaging study, the animals were injected with a 0.2-ml bolus of 3.3 MBq-labeled ET-1. The specific activity at the time of each study was usually ~200 GBq/µmol (5.4 Ci/µmol). The lungs, heart, liver, and kidney of the animals were monitored for [^18^F]ET-1 uptake. Only the lungs and kidneys showed a high uptake of the label. In the liver, only a moderate uptake was observed. Results for the heart were not presented (11). These observations indicated that organs showing an accumulation of the tracer have ET receptors, and, among these, the lungs and kidneys were possibly responsible for clearing ET-1 from circulation (11). A similar suggestion was made earlier by Fukuroda et al (17), who used ^125^I-labeled ET-1 in competition studies with selective ET_A_ and ET_B_ receptor antagonists. Statements about specific binding to ER receptors can only be made if the authors did blocking studies with cold ET.

In another in vivo study in rats from the same laboratory (10), which was followed by ex vivo analysis, an accumulation of radioactivity was observed mainly in the lung, liver, kidney, and bladder. The thyroid, pituitary, and salivary glands showed low uptake. No uptake was observed in the brain or bone. In this study, [^125^I]ET-1 was used for comparison. Observations from the in vivo study correlated with the in vitro detection of receptors in the lung, liver, and kidney as observed with [^125^I]ET-1. The binding of [^18^F]ET-1 in the lung could not be displaced by BQ788, a selective ET_B_ receptor antagonist. However, infusion of BQ788 prior to treatment with [^18^F]ET-1 significantly reduced the uptake of radioactivity in the lung (85% reduction) and kidney (55% reduction). Under these conditions some uptake was observed in the heart. Only in the heart was the binding lower than expected, as observed with [^125^I]ET-1 during in vitro studies (18). Evidently, [^18^F]ET-1 had a rapid clearance from circulation with a half-life of 0.43 min, and a simultaneous increase in radioactivity was observed in the liver and lungs. These organs showed high levels of radioactivity up to 2 hr after administration. In the kidney the uptake was initially rapid and after 20 min it increased slowly. The investigators suggest this could be caused by the accumulation of [^18^F]ET-1 metabolites in the organ.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20non-primate%20mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20non-human%20primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20endothelin%20human%20studies)]

No publications are currently available.

## References

1 Kedzierski RM, Yanagisawa M. (2001). Endothelin system: the double-edged sword in health and disease. Annu Rev Pharmacol Toxicol.
2 Miyauchi T, Masaki T. (1999). Pathophysiology of endothelin in the cardiovascular system. Annu Rev Physiol.
3 Schiffrin EL, Intengan HD, Thibault G, Touyz RM. (1997). Clinical significance of endothelin in cardiovascular disease. Curr Opin Cardiol.
4 Arai H, Hori S, Aramori I, Ohkubo H, Nakanishi S. (1990). Cloning and expression of a cDNA encoding an endothelin receptor. Nature.
5 Sakurai T, Yanagisawa M, Takuwa Y, Miyazaki H, Kimura S, Goto K, Masaki T. (1990). Cloning of a cDNA encoding a non-isopeptide-selective subtype of the endothelin receptor. Nature.
6. Davenport, AP, Distribution of endothelin receptors. Endothelins in biology and medicine., ed. JP Huggins and JT Pelton. 1997, Boca Raton: CRC Press, Inc. 45-68.
7 de Nucci G, Thomas GR, D'Orleans-Juste P, Antunes E, Walder C, Warner TD, Vane JR. (1988). Pressor effects of circulating endothelin are limited by its removal in primary circulation and by the release of prostacyclin and endothelium-derived relaxing factor. Proc. Natl. Acad. Sci. USA.
8 Yokokawa K, Tahara H, Kohno M, Murakawa K, Yasunari K, Nakagawa K, Hamada T, Otani S, Yanagisawa M, Takeda T. (1991). Hyperstension associated with endothelin secreting malignant hemangioendothelioma. Ann Intern Med.
9 Johnstrom P, Fryer TD, Richards HK, Barret O, Clark JC, Ohlstein EH, Pickard JD, Davenport AP. (2004). In Vivo Imaging of Cardiovascular Endothelin Receptors Using the Novel Radiolabelled Antagonist [18F]-SB209670 and Positron Emission Tomography (microPET). J Cardiovasc Pharmacol.
10 Johnstrom P, Fryer TD, Richards HK, Harris NG, Barret O, Clark JC, Pickard JD, Davenport AP. (2005). Positron emission tomography using 18F-labelled endothelin-1 reveals prevention of binding to cardiac receptors owing to tissue-specific clearance by ET B receptors in vivo. Br J Pharmacol.
11 Johnstrom P, Harris NG, Fryer TD, Barret O, Clark JC, Pickard JD, Davenport AP. (2002). (18)F-Endothelin-1, a positron emission tomography (PET) radioligand for the endothelin receptor system: radiosynthesis and in vivo imaging using microPET. Clin Sci (Lond).
12 Johnstrom P, Rudd JH, Richards HK, Fryer TD, Clark JC, Weissberg PL, Pickard JD, Davenport AP. (2006). Imaging endothelin ET(B) receptors using [18F]-BQ3020: in vitro characterization and positron emission tomography (microPET). Exp Biol Med (Maywood).
13 Johnstrom P Aigbirhio FI Clark JC Downey SP Pickard JD Davenport AP Syntheses of the first endothelin-A- and -B-selective radioligands for positron emission tomography J Cardiovasc Pharmacol 2000 36 Suppl 1 5 S58 60 11078336
14 Vaidyanathan G, Zalutsky MR. (1992). Labeling proteins with fluorine-18 using N-succinimidyl 4-[18F]fluorobenzoate. Int J Rad Appl Instrum B.
15 Wester HJ, Hamacher K, Stocklin G. (1996). A comparative study of N.C.A. fluorine-18 labeling of proteins via acylation and photochemical conjugation. Nucl Med Biol.
16 Davenport AP, Kuc RE. (2002). Radioligand binding assays and quantitative autoradiography of endothelin receptors. Methods Mol biol.
17 Fukuroda T, Fujikawa T, Ozaki S, Ishikawa K, Yano M, Nishikibe M. (1994). Clearance of circulating endothelin-1 by ETB receptors in rats. Biochem Biophys Res Commun.
18 Molenaar P, O'Reilly G, Sharkey A, Kuc RE, Harding DP, Plumpton C, Gresham GA, Davenport AP. (1993). Characterization and localization of endothelin receptor subtypes in the human atrioventricular conducting system and myocardium. Circ Res.